# Alexa Fluor 750-albumin-binding domain-fused-(Z_HER2:342_)_2_ Affibody

Chemical name: | Alexa Fluor 750-albumin-binding domain-fused-(Z_HER2:342_)_2_ Affibody
Abbreviated name: | Alexa750-ABD-fused-(Z_HER2:342_)_2_ Affibody
Synonym:
Agent category: | Antibody
Target: | EGF HER2 receptor
Target category: | Receptor
Method of detection: | Optical, near-infrared fluorescence (NIR) imaging
Source of signal: | Alexa Fluor 750
Activation: | No
Studies: | - In vitro; - Rodents | No structure is available in PubChem.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20Alexa)]

Epidermal growth factor (EGF) is a 53-amino acid cytokine (6.2 kDa) secreted by ectodermic cells, monocytes, kidneys and duodenal glands (1). EGF stimulates growth of epidermal and epithelial cells. EGF with at least seven other growth factors and their transmembrane receptor kinases play important roles in cell proliferation, survival, adhesion, migration and differentiation. The EGF receptor (EGFR) family consists of four transmembrane receptors, including EGFR (HER1/erbB-1), HER2 (erbB-2/neu), HER3 (erbB-3) and HER4 (erbB-4) (2). HER1, HER3 and HER4 comprise three major functional domains: an extracellular ligand-binding domain, a hydrophobic transmembrane domain and a cytoplasmic tyrosine kinase domain. No ligand has been clearly identified for HER2. However, HER2 can be activated as a result of ligand binding to other HER receptors with the formation of receptor homodimers and/or heterodimers (3). HER1 as well as HER2 are overexpressed on many solid tumor cells such as breast, non-small-cell lung, head and neck, and colon cancer (4-6). The high levels of HER1 and HER2 expression on cancer cells are associated with a poor prognosis (7-10).

Trastuzumab is a humanized IgG_1_ monoclonal antibody (mAb) against the extracellular domain of recombinant HER2 with an affinity constant (K_d_) of 0.1 nM (11). ^111^In-Trastuzumab, Cy5.5-trastuzumab, and ^68^Ga-trastuzumab-F(ab')_2_ have been developed for imaging of human breast cancer (12-16). However, the pharmacokinetics of intact radiolabeled mAb, with high liver uptake and slow blood elimination, are generally not ideal for imaging. Smaller antibody fragments, such as Fab or F(ab´)_2_, have better imaging pharmacokinetics because they are rapidly excreted by the kidneys. A novel class of recombinant affinity ligands (Affibody molecules) for HER2 was constructed based on a 58-amino-acid Z-domain residues from one of the IgG-binding domains of staphylococcal protein A (17). Affibody molecules exhibit high binding affinity to HER2 with K_d_ values of <50 nM. Various radiolabeled Affibody molecules have been studied in their ability for imaging of HER2 in tumors [PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=affibody%20and%20HER2)]. A synthetic Affibody molecule was successfully made as albumin-binding domain (ABD)-fused-(Z_HER2:342_)_2_ Affibody dimer for labeling with Alexa Fluor 750 (Alexa750) (18). Alexa750-ABD-(Z_HER2:342_)_2_ has been evaluated in nude mice bearing human SKBR-3 breast adenocarcinoma tumor.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=HER2+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (HER2 (http://www.ncbi.nlm.nih.gov/sites/entrez?db=gene&cmd=Retrieve&dopt=full_report&list_uids=2064)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=HER2)
- Clinical trials (Trastuzumab (http://www.clinicaltrials.gov/ct2/results?term=Trastuzumab))
- Drug information in FDA (Trastuzumab (http://google2.fda.gov/search?q=Trastuzumab&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=11&y=14))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20Alexa%20and%20synthesis)]

ABD-(Z_HER2:342_)_2_-Cys was incubated with 5 nM neutral tris(2-carboxyethyl)phosphine solution at room temperature for 20 min (18). Immediately after the reduction, thio-reactive dye Alexa Fluor 750-maleimide was added to the mixture. Alexa750-ABD-(Z_HER2:342_)_2_ was purified by column chromatography with an estimated labeling efficiencies of 60-80%, assuming a 1:1 conjugation. Alexa480- and Alexa750- Z_HER2:342_ were also prepared similarly.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20Alexa%20and%20in%20vitro)]

Lee et al. (18) performed binding experiments with Z_HER2:342_ and Z_HER2:342_-Alexa Fluor 750 using a Biacore sensor chip immobilized with extracellular domain of chimeric HER2/Fc fusion protein. The dissociation constants (K_d_ ) of Z_HER2:342_ were calculated to be 30 pM for chimeric HER2/Fc fusion protein. The K_d_ value of Z_HER2:342_-Alexa Fluor 750 was 190 pM. Hence, the binding affinity of the synthetic Affibody molecule Z_HER2:342_-Alexa Fluor 750 was ~5 folds lower than the recombinant Affibody molecule Z_HER2:342_. Binding specificity tests in vitro showed that binding of 5 nM Z_HER2:342_-Alexa480 to SKOV-3 cells expressing HER2 was receptor mediated because saturation of receptors by preincubation with non-labeled Z_HER2:342_ and trastuzumab decreased binding of Z_HER2:342_-Alexa Fluor 480 by 97% and 98%, respectively. Confocal microscopy confirmed cellular internalization of both Z_HER2:342_-Alexa480 and trastuzumab-Alexa680.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20Alexa%20and%20rodentia)]

Lee et al. (18) monitored biodistribution using NIR optical imaging of HER2-expressing SKBR-3 tumor xenograft mice (n = 3/group) after intravenous injection of 10 µg Alexa750-ABD-(Z_HER2:342_)_2_, 10 µg Alexa750-Z_HER2:342_, or 50 µg Alexa750-trastuzumab. Tumor fluorescence intensities were measured at 1, 8, 24, and >48 h after tracer injection. Alexa750-ABD-(Z_HER2:342_)_2_ showed high signals around the tumor and kidney area at 8 h after injection. Fluorescence signals in the tumor area peaked ~24 h (3.6 AU) and decreased gradually to background level at 72 h. The organ with the highest concentration was the kidney (3.7 AU), followed by the liver (1.3 AU), heart (0.6 AU), lung (0.5 AU) and muscle (0.3 AU). Pre-administration of ABD-(Z_HER2:342_)_2_ (1 mg/mouse) 30 min before Alexa750-ABD-(Z_HER2:342_)_2_ injection resulted in decreased uptake in the tumor. On the other hand, Alexa750-trastuzumab exhibited moderate fluorescence intensity in the tumor, which peaked at ~48 h. Alexa750-Z_HER2:342_ exhibited a high initial accumulation in the tumor with a fast washout. The tumor clearance rates (t_½_) of Alexa750-ABD-(Z_HER2:342_)_2_, Alexa750-Z_HER2:342_, and Alexa750-trastuzumab were 40.5, 5.7, and 115 h, respectively. The maximum tumor/muscle ratios were 4.5 at 48 h for the dimer, 2.5 at 4 h for monomer, and 2.5 at 48 h for the intact trastuzumab antibody.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20Alexa%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20Alexa%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=Affibody%20Alexa%20and%20human)]

No publication is currently available.

## NIH support

Intramural Research Program, N01-CO-12400, N01-CO-12401

## References

1 Carpenter G., Cohen S. (1990). Epidermal growth factor. J Biol Chem.
2 Yarden Y. (2001). The EGFR family and its ligands in human cancer. signalling mechanisms and therapeutic opportunities. Eur J Cancer.
3 Rubin I., Yarden Y. (2001). The basic biology of HER2. Ann Oncol.
4 Grunwald V., Hidalgo M. (2003). Developing inhibitors of the epidermal growth factor receptor for cancer treatment. J Natl Cancer Inst.
5 Mendelsohn J. (1990). Anti-epidermal growth factor receptor monoclonal antibodies as potential anti-cancer agents. J Steroid Biochem Mol Biol.
6 Yasui W., Sumiyoshi H., Hata J., Kameda T., Ochiai A., Ito H., Tahara E. (1988). Expression of epidermal growth factor receptor in human gastric and colonic carcinomas. Cancer Res.
7 Ang K.K., Berkey B.A., Tu X., Zhang H.Z., Katz R., Hammond E.H., Fu K.K., Milas L. (2002). Impact of epidermal growth factor receptor expression on survival and pattern of relapse in patients with advanced head and neck carcinoma. Cancer Res.
8 Costa S., Stamm H., Almendral A., Ludwig H., Wyss R., Fabbro D., Ernst A., Takahashi A., Eppenberger U. (1988). Predictive value of EGF receptor in breast cancer. Lancet.
9 Ethier S.P. (1995). Growth factor synthesis and human breast cancer progression. J Natl Cancer Inst.
10 Yarden Y. (2001). Biology of HER2 and its importance in breast cancer. Oncology.
11 Carter P., Presta L., Gorman C.M., Ridgway J.B., Henner D., Wong W.L., Rowland A.M., Kotts C., Carver M.E., Shepard H.M. (1992). Humanization of an anti-p185HER2 antibody for human cancer therapy. Proc Natl Acad Sci U S A.
12 Perik P.J., Lub-De Hooge M.N., Gietema J.A., van der Graaf W.T., de Korte M.A., Jonkman S., Kosterink J.G., van Veldhuisen D.J., Sleijfer D.T., Jager P.L., de Vries E.G. (2006). Indium-111-labeled trastuzumab scintigraphy in patients with human epidermal growth factor receptor 2-positive metastatic breast cancer. J Clin Oncol.
13 Lub-de Hooge M.N., Kosterink J.G., Perik P.J., Nijnuis H., Tran L., Bart J., Suurmeijer A.J., de Jong S., Jager P.L., de Vries E.G. (2004). Preclinical characterisation of 111In-DTPA-trastuzumab. Br J Pharmacol.
14 Garmestani K., Milenic D.E., Plascjak P.S., Brechbiel M.W. (2002). A new and convenient method for purification of 86Y using a Sr(II) selective resin and comparison of biodistribution of 86Y and 111In labeled Herceptin. Nucl Med Biol.
15 Smith-Jones P.M., Solit D., Afroze F., Rosen N., Larson S.M. (2006). Early tumor response to Hsp90 therapy using HER2 PET: comparison with 18F-FDG PET. J Nucl Med.
16 Smith-Jones P.M., Solit D.B., Akhurst T., Afroze F., Rosen N., Larson S.M. (2004). Imaging the pharmacodynamics of HER2 degradation in response to Hsp90 inhibitors. Nat Biotechnol.
17 Wikman M., Steffen A.C., Gunneriusson E., Tolmachev V., Adams G.P., Carlsson J., Stahl S. (2004). Selection and characterization of HER2/neu-binding affibody ligands. Protein Eng Des Sel.
18 Lee S.B., Hassan M., Fisher R., Chertov O., Chernomordik V., Kramer-Marek G., Gandjbakhche A., Capala J. (2008). Affibody molecules for in vivo characterization of HER2-positive tumors by near-infrared imaging. Clin Cancer Res.